# ^99m^Tc-Ethylenedicysteine-guanine

Chemical name: | ^99m^Tc- Ethylenedicysteine-guanine
Abbreviated name: | ^99m^Tc-EC-Guan
Synonym: | N-[4-(2-amino-6-oxo-4,5-dihydro-1H-purin-9-yl)-2-(hydroxymethyl)butyl]-2-[2-[(1-amino-1-oxo-3-sulfanylpropan-2-yl)amino]ethylamino]-3-sulfanylpropanamide
Agent Category: | Compound
Target: | Thymidine kinase
Target Category: | DNA incorporation
Method of detection: | Single-photon emission computed tomography or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | Not required
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Ethylenedicysteine+guanine)]

Evaluation of tumor malignancy and growth potential is important for the assessment of cancer treatment. For this evaluation, the uptake of indicators such as ^18^F-labeled 2’-fluorodeoxyglucose (^18^F-FDG) is often used to monitor the effectiveness of a treatment because ^18^F-FDG was shown to be related to the number of viable cells present in a tumor (1, 2). In addition, a variety of labeled amino acids have also been used to determine the proliferative potential of neoplastic cells and tumors (3, 4). Although these compounds determine the proliferation of viable cells, none of them are incorporated into the cellular DNA and can not determine the true state of tumor malignancy and proliferative potential. Because labeled purine- and pyramidine-based compounds can be incorporated into DNA, these agents can be employed to determine tumor malignancy and proliferative potential, and to evaluate the efficacy of or response to a treatment. However, a variety of ^18^F-labeled pyrmidine or purine compounds have been used primarily to image the expression of reporter genes such as the wild-type or mutant herpes simplex virus type I thymidine kinase (HSV1-tk) (5, 6). The thymidine kinase enzyme (TK) produced from HSV-tk phosphorylates many different substrates, including acycloguanines. Because mammalian TK is known to minimally phosphorylate acycloguanines, this makes such compounds useful only for the imaging of reporter genes (6).

To assess the efficacy of tumor therapy, it is important to have an agent that interacts primarily with the endogenous TK and measures only cell proliferation. Different isotopes of carbon (^11^C), iodine (^123/125^I), or fluorine (^18^F) have been employed to generate labeled thymidine or uracil for the investigation of cell proliferation because these compounds are incorporated into cellular DNA or RNA (7-9). Nonetheless, these compounds have limited use either because of the complex chemistry involved in their synthesis, short isotope half-life, or stability issues. Because technetium (^99m^Tc) has a longer half-life than ^11^C, ^123/125^I, or ^18^F, Yang et al. synthesized a ^99m^Tc-labeled guanine (a purine) analog that contains ethylenedicysteine (EC) as a chelator of ^99m^Tc (10). Subsequently, ^99m^Tc-EC-guanine (^99m^Tc-EC-guan) was investigated for the biodistribution and assessment of tumor growth in rodents (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+Guan+synthesis)]

For the synthesis of ^99m^Tc-EC-guan, 9-[4-amino-3-(hydroxymethyl)butyl]guanine (compound I) was synthesized first (10). For this, N^2^-(p-anisyldiphenylmethyl)-9-[(4-tosyl)-3-p-anisyldiphenylmethoxymethylbutyl]guanine was dissolved in N,N-dimethylformamide, and sodium azide was added to the mixture. The mixture was heated to 100°C and stirred for 2 h; then the mixture was cooled to room temperature, and the solvent was evaporated under reduced pressure to 25% of the original volume. Ethyl acetate and water were added to the residue, which was then agitated and allowed to separate into the organic and aqueous phases. The aqueous layer was washed twice with ethyl acetate, and the two extractions were pooled. The pooled extractions were then washed with water and dried over anhydrous magnesium sulphate. The solvent was filtered and evaporated to dryness to obtain a crude azido compound. The crude compound was dissolved in tetrahydrofuran, and triphenylphosphine was added to it. This mixture was stirred overnight at room temperature and 5 N hydrochloric acid was added to it. The mixture was then heated under reflux for 5 h, filtered, and evaporated to dryness. The residue was mixed with water and washed with ethyl acetate, and the pH was adjusted to between 7 and 8 with 1 N sodium hydroxide. The product solution was isolated by column chromatography on a Sephadex G-15 column. The chromatographed solution was freeze-dried to obtain compound I. The yield of this reaction was 76.2%.

The EC was conjugated to compound I essentially as described in detail elsewhere (11, 12). Briefly, 1 N sodium hydroxide and 1 N sodium bicarbonate were mixed with a solution of EC. Subsequently, compound I, N-hydroxysulfosuccinimide, and 1-ethyl-3-(3-dimethylaminoethyl)carbodiimide were added to the solution mixture. The mixture was stirred at room temperature overnight. The mixture was dialyzed for 24 h and the product was freeze-dried to obtain EC-guan with a yield of 40%.

To label EC-guan with ^99m^Tc, EC-guan was dissolved in water and tin (II) chloride solution was added. Sodium pertechnetate and water were added to the mixture to a volume of 1 mL. Radiochemical purity of the labeled compound was determined to be >97% by instant thin-layer chromatography (Rf 0.8). The specific activity of the labeled compound was not provided.

For some studies, ^99m^Tc-EC and ^18^F-FDG were used as controls. The synthesis, radiochemical purity, specific activity, and Rf values for these compounds were not provided.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+Guan+in+vitro+studies)

To determine if ^99m^Tc-EC-guan could be used for the assessment of tumor growth, the uptake of this radiochemical was investigated in three human cancer cell lines: NSCLC A549 (of lung origin), OCA3 (ovarian cells), and PC-3 (prostate cell line) (10). To show that ^99m^Tc-EC-guan was independent of the HSV-TK gene–mediated process, the PC-3 cells were transfected with an adeno-associated virus vector containing the HSV-tk and β-galactosidase genes. No differences in the uptake of ^99m^Tc-EC-guan were noted in the untransfected or transfected cells, which indicated that uptake of the radiochemical was independent of the HSV-tk gene and so the radiochemical could be used for the assessment of cell proliferation.

In another study, the uptakes of ^99m^Tc-EC-guan, ^99m^Tc-EC, and ^18^F-FDG were compared in the lung cell line sorted by fluorescence-activated cell-cycle phase sorting (10). Compared to ^99m^Tc-EC and ^18^F-FDG, which showed a low uptake (<0.1% of the total dose), a high uptake of ^99m^Tc-EC-guan (2.5% of the total dose) was observed in the S-phase cells that actively synthesize DNA. Results from the uptake studies with the transfected cells and ^99m^Tc-EC, ^99m^Tc-EC-guan, and ^18^F-FDG indicated that the uptake of ^99m^Tc-EC-guan was specific to the cell cycle and independent of the HSV-tk gene, which suggested that the radiochemical could be used for the assessment of tumor growth in animals.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+Guan+rodentia)]

The biodistribution of ^99m^Tc-EC and ^99m^Tc-EC-guan was investigated in two separate groups of rats (n = 9 animals in each group) bearing rat breast adenocarcinoma cell tumors (10). The animals were injected with the respective radiotracers and euthanized at 0.5, 2, and 4 h after injection (n = 3 animals for each time point). The various tissues were removed, weighed, and counted for radioactivity. Maximum radioactivity from ^99m^Tc-EC-guan, calculated as a percentage of injected dose per gram (% ID/g), was compared to ^99m^Tc-EC and used to determine the tumor/blood and tumor/nontarget (muscle) count density ratios. Although both ratios increased as a function of time for the two radiochemicals, the accumulation of ^99m^Tc-EC-guan in the tumors was found by t test to be significantly higher than ^99m^Tc-EC at any time point (P < 0.05).

Whole-body autoradiographic studies were performed with nude mice bearing ovarian cell cancer tumors to show that ^99m^Tc-EC-guan could be used to determine the change in tumor volume before and after treatment with paclitaxel, an anti-cancer drug (10). Although different animals were used for the pre- and post-treatment groups, all animals used in the study had similar baseline tumor volumes. All animals were euthanized 1 h after injection with ^99m^Tc-EC-guan, and the bodies were frozen and fixed in carboxymethyl cellulose for autoradiography with a quantitative image analyzer. Although no quantitative data was provided in the publication, the investigators mentioned that no enlargement of the tumor in the paclitaxel-treated mice was observed. This indicated that ^99m^Tc-EC-guan could be used for the determination of tumor growth.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+Guan+Non-Primate+Mammals)]

Planar scintigraphic imaging studies were performed with ^99m^Tc-EC-guan in rabbits (10). The animals were intramuscularly inoculated in the hind thighs with VX2 squamous carcinoma cells (of lung origin), and imaging studies were performed 12–15 days after the inoculation. Planar scintigraphy was performed 0.5–3.5 h after i.v. injection of either ^99m^Tc-EC or ^99m^Tc-EC-guan. The tumor/muscle ratios for the radiochemicals were 3.05–3.96 and 2.46– 2.71, respectively, at 1–3.5 h. The investigators cautioned that although ^99m^Tc-EC-guan could be used to observe tumors in the legs, detection of tumors in the body cavity may not be possible because the interference of background signal from internal organs.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+Guan+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+Guan+Human+Studies)]

No publications are currently available.

## References

1 Higashi K., Clavo A.C., Wahl R.L. (1993). Does FDG uptake measure proliferative activity of human cancer cells? In vitro comparison with DNA flow cytometry and tritiated thymidine uptake. J Nucl Med.
2 Okada J., Yoshikawa K., Itami M., Imaseki K., Uno K., Itami J., Kuyama J., Mikata A., Arimizu N. (1992). Positron emission tomography using fluorine-18-fluorodeoxyglucose in malignant lymphoma: a comparison with proliferative activity. J Nucl Med.
3 Jager P.L., Plaat B.E., de Vries E.G., Molenaar W.M., Vaalburg W., Piers D.A., Hoekstra H.J. (2000). Imaging of soft-tissue tumors using L-3-[iodine-123]iodo-alpha-methyl-tyrosine single photon emission computed tomography: comparison with proliferative and mitotic activity, cellularity, and vascularity. Clin Cancer Res.
4 McConathy J., Martarello L., Malveaux E.J., Camp V.M., Simpson N.E., Simpson C.P., Bowers G.D., Zhang Z., Olson J.J., Goodman M.M. (2003). Synthesis and evaluation of 2-amino-4-[(18)F]fluoro-2-methylbutanoic acid (FAMB): relationship of amino acid transport to tumor imaging properties of branched fluorinated amino acids. Nucl Med Biol.
5 Tjuvajev J.G., Doubrovin M., Akhurst T., Cai S., Balatoni J., Alauddin M.M., Finn R., Bornmann W., Thaler H., Conti P.S., Blasberg R.G. (2002). Comparison of radiolabeled nucleoside probes (FIAU, FHBG, and FHPG) for PET imaging of HSV1-tk gene expression. J Nucl Med.
6 Gambhir S.S., Bauer E., Black M.E., Liang Q., Kokoris M.S., Barrio J.R., Iyer M., Namavari M., Phelps M.E., Herschman H.R. (2000). A mutant herpes simplex virus type 1 thymidine kinase reporter gene shows improved sensitivity for imaging reporter gene expression with positron emission tomography. Proc Natl Acad Sci U S A.
7 Goethals P., van Eijkeren M., Lodewyck W., Dams R. (1995). Measurement of [methyl-carbon-11]thymidine and its metabolites in head and neck tumors. J Nucl Med.
8 Tjuvajev J.G., Macapinlac H.A., Daghighian F., Scott A.M., Ginos J.Z., Finn R.D., Kothari P., Desai R., Zhang J., Beattie B., et al. (1994). Imaging of brain tumor proliferative activity with iodine-131-iododeoxyuridine. J Nucl Med.
9 Abe Y., Fukuda H., Ishiwata K., Yoshioka S., Yamada K., Endo S., Kubota K., Sato T., Matsuzawa T., Takahashi T., Ido T. (1983). Studies on 18F-labeled pyrimidines. Tumor uptakes of 18F-5-fluorouracil, 18F-5-fluorouridine, and 18F-5-fluorodeoxyuridine in animals. Eur J Nucl Med.
10 Yang D.J., Ozaki K., Oh C.S., Azhdarinia A., Yang T., Ito M., Greenwell A., Bryant J., Kohanim S., Wong V.K., Kim E.E. (2005). (99m)Tc-EC-guanine: synthesis, biodistribution, and tumor imaging in animals. Pharm Res.
11 Song H.C., Bom H.S., Cho K.H., Kim B.C., Seo J.J., Kim C.G., Yang D.J., Kim E.E. (2003). Prognostication of recovery in patients with acute ischemic stroke through the use of brain SPECT with Technetium-99m--labeled metronidazole. Stroke.
12 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.